# Humanized anti–type 1 insulin-like growth factor receptor monoclonal antibody conjugated to cadmium telluride quantum dots

Chemical name: | Humanized anti–type 1 insulin-like growth factor receptor monoclonal antibody conjugated to cadmium telluride quantum dots
Abbreviated name: | AVE1642-QD
Synonym:
Agent Category: | Antibody
Target: | Type 1 insulin-like growth factor receptor (IGF1R)
Target Category: | Receptor
Method of detection: | Near-infrared (NIR) fluorescence
Source of signal / contrast: | Quantum dots (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ave1642)]

Overexpression and activation of the type 1 insulin-like growth factor receptor (IGF1R), which mediates its activity through an associated tyrosine kinase, is believed to promote the progression and metastasis of several cancers (1-3). In addition, higher than normal or overexpression of the IGF1R itself, or any of its different constituent parts, is considered to indicate an aggressive or drug-resistant cancer phenotype with a poor prognosis for the patient (3). As a consequence, the IGF1R is a target of various agents, including monoclonal antibodies (mAbs) directed against it, that are under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=IGF1R) approved by the United States Food and Drug Administration for the treatment of cancers. Also, using xenograft tumor models, a downregulation in IGF1R expression has been shown to be accompanied by reduced tumor growth, suggesting that IGF1R levels can be used to monitor patient response to anti-cancer treatment(s) (4, 5).

The epidermal growth factor receptor (EGFR), which is known to be overexpressed in several cancers, is routinely quantified in a clinical setting with in situ hybridization or immunohistochemical techniques, and the data obtained from these investigations are used to select patients who are most likely to benefit from an anti-EGFR therapy (6, 7). However, no such quantification is available for IGF1R expression, which has been quantified only in cultured cells using a humanized anti-IGF1R mAb (AVE1642) conjugated to cadmium telluride quantum dots (QD) (AVE1642-QD) (8). Recently, the use of AVE1642 QD was evaluated for the detection and imaging of xenograft tumors that express IGF1R in a mouse model (9). For comparison, the investigators also evaluated the use of Alexa 680 (a near-infrared fluorescent dye with a maxima at 705 nm) covalently linked to AVE1642 (AVE1642-Alexa 680) (discussed in a separate chapter of MICAD; www.micad.nih.gov) for the detection and imaging of the tumors expressing IGF1R (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+synthesis)]

The AVE1642 mAb was obtained from a commercial source, and its conjugation with the QDs was performed with a heterobifunctional cross-linker, succinimidyl-4-(N-maleimidomethyl)cyclohexane-1-carboxylate, as described by Zhang et al. (9). Purification of the AVE1642-QD conjugate was not described. The number of AVE1642 molecules conjugated to each QD and the stability of the complex under in vitro or in vivo conditions were not reported.

For one of the studies, an alternate method, which generated a direct-linkage between the mAb and the QDs, was used to generate the AVE1642-QDs (9). The purification, number of AVE1642 molecules linked to each QD, and stability of the complex were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+in+vitro)]

The receptor binding ability of AVE1642-QD was investigated using mouse embryo fibroblast R-/IGF1R cells (R cells stably transfected with human igf1r DNA) that express high levels of IGF1R (9). The cells were exposed to either AVE1642-QD, QD alone (control), or an anti-CD20 antibody conjugated to the QD (negative control) for 1 h at 4°C in phosphate-buffered saline (PBS) containing 1% bovine serum albumin and 0.1% sodium azide. Binding of the fluorescent mAbs or the QDs was analyzed with fluorescence-assisted cell sorting (FACS). Only cells exposed to AVE1642-QD were reported to show fluorescence, and no signal was obtained from cells exposed to the unconjugated QDs. R-/IGF1R cells pretreated with AVE1642 did not produce a fluorescent signal upon exposure to the QD conjugated mAb, indicating that the cells had downregulated the IGF1R levels due to prior exposure to AVE1642.

In another study, MCF-7 cells, a breast cancer cell line that constitutively expresses high levels of the IGF1R, were shown with FACS analysis to bind AVE1642-QD but not QDs alone (9).

From these studies the investigators concluded that AVE1642-QD was able to detect the expression of IGF1R under in vitro conditions (9). These observations were similar to those obtained with the AVE1642-Alexa680 conjugate (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+rodentia)]

Zhang et al. used athymic mice bearing xenograft tumors generated with R-/IGF1R cells to investigate the in vivo specificity of AVE1642-QD (9). The mice were injected with 0.1 nmol of the QD-conjugated mAb through the tail vein (control animals were injected with PBS alone), and blood was drawn from the animals at predesignated time points (the number of animals used per time point was not reported) to determine the QD fluorescence by imaging. The QD fluorescence of blood was reported to diminish very rapidly, and by 2 h after treatment no fluorescence was detectable in this organ. On the basis of this observation, for subsequent work, whole-body imaging of the animals was performed only at 2 and 24 h after mAb-QD conjugate injection. By 2 h after the conjugate treatment, QD fluorescence was observed primarily in organs that contain the reticuloendothelial system (RES) and are rich in phagocytic cells (e.g., liver, bone marrow, lymph nodes, and spleen). The high nonspecific uptake of QDs by these organs was reported to mask the fluorescent signal from the tumors in the animals. Ex vivo imaging of the tumors revealed that the fluorescent signal was present in the middle of tumors obtained from the animals injected with either the QDs alone or the animals injected with the QD-conjugated mAb. In addition, there was little difference between the fluorescence obtained from the tumors of both animal groups. Pretreatment of the animals with AVE1642 before injection with AVE1642-QD did not reduce the fluorescence in tumors from either group. From these observations the investigators concluded that, although the QDs and the AVE1642-QDs accumulated in the tumors, the uptake of these agents was nonspecific and independent of IGF1R expression (9).

Ex vivo imaging of tumors performed with the QDs and with the mAb-QD complex generated by an alternate method (see the Synthesis section above for details) yielded results similar to those detailed above (9). This confirmed that the tumor uptake of AVE1642-QD was due to nonspecific binding of the complex to the cells and did not depend on the level of IGF1R expressed by the cells.

Toluidine blue staining of liver sections obtained from animals treated with AVE1642-QD showed that the mAb-QD complex was localized in the liver sinusoids at 2 and 24 h after treatment of the animals (9). Staining of the liver sections with an antibody directed specifically against the monocytes and the macrophages (MOMA-2) showed that the AVE1642-QD fluorescence was co-localized with the MOMA-2 staining of the sections. Treatment of the animals with clodronate liposomes, which are known to deplete macrophages from the RES of the organs, did not prevent the uptake of AVE1642-QD by the liver cells. This indicated that uptake of the mAb-QD complex in the liver was independent of macrophage accumulation in RES of the organ.

From these studies the investigators concluded that AVE1642-QD performed well only under in vitro conditions, but could not be used in vivo for the detection and quantification of IGF1R in a rodent model (9). In comparison, AVE1642-Alexa680 was shown to be a suitable imaging agent to detect and quantify IGF1R under in vivo conditions (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 McCampbell A.S., Broaddus R.R., Loose D.S., Davies P.J. (2006). Overexpression of the insulin-like growth factor I receptor and activation of the AKT pathway in hyperplastic endometrium. Clin Cancer Res.
2 Yuen J.S., Akkaya E., Wang Y., Takiguchi M., Peak S., Sullivan M., Protheroe A.S., Macaulay V.M. (2009). Validation of the type 1 insulin-like growth factor receptor as a therapeutic target in renal cancer. Mol Cancer Ther.
3 Hewish M., Chau I., Cunningham D. (2009). Insulin-like growth factor 1 receptor targeted therapeutics: novel compounds and novel treatment strategies for cancer medicine. Recent Pat Anticancer Drug Discov.
4 Goetsch L., Gonzalez A., Leger O., Beck A., Pauwels P.J., Haeuw J.F., Corvaia N. (2005). A recombinant humanized anti-insulin-like growth factor receptor type I antibody (h7C10) enhances the antitumor activity of vinorelbine and anti-epidermal growth factor receptor therapy against human cancer xenografts. Int J Cancer.
5 Shang Y., Mao Y., Batson J., Scales S.J., Phillips G., Lackner M.R., Totpal K., Williams S., Yang J., Tang Z., Modrusan Z., Tan C., Liang W.C., Tsai S.P., Vanderbilt A., Kozuka K., Hoeflich K., Tien J., Ross S., Li C., Lee S.H., Song A., Wu Y., Stephan J.P., Ashkenazi A., Zha J. (2008). Antixenograft tumor activity of a humanized anti-insulin-like growth factor-I receptor monoclonal antibody is associated with decreased AKT activation and glucose uptake. Mol Cancer Ther.
6 Meche A., Cimpean A.M., Raica M. (2009). Immunohistochemical expression and significance of epidermal growth factor receptor (EGFR) in breast cancer. Rom J Morphol Embryol.
7 Martin V., Mazzucchelli L., Frattini M. (2009). An overview of the epidermal growth factor receptor fluorescence in situ hybridisation challenge in tumour pathology. J Clin Pathol.
8 Zhang H., Sachdev D., Wang C., Hubel A., Gaillard-Kelly M., Yee D. (2009). Detection and downregulation of type I IGF receptor expression by antibody-conjugated quantum dots in breast cancer cells. Breast Cancer Res Treat.
9 Zhang H., Zeng X., Li Q., Gaillard-Kelly M., Wagner C.R., Yee D. (2009). Fluorescent tumour imaging of type I IGF receptor in vivo: comparison of antibody-conjugated quantum dots and small-molecule fluorophore. Br J Cancer.